# ^177^Lu-Labeled methylene diphosphonate

Chemical name: | ^177^Lu-Labeled methylene diphosphonate | [image]
Abbreviated name: | [^177^Lu]-MDP | [image]
Synonym: | | [image]
Agent Category: | Compound | [image]
Target: | Type 2 class of aminoacyl-tRNA synthetases | [image]
Target Category: | Enzyme | [image]
Method of detection: | Single-photon emission tomography (SPECT); gamma planar imaging | [image]
Source of signal / contrast: | ^177^Lu | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of methylene diphosphonate.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=methylene%20diphosphonate&cmd=DetailsSearch)]

Most patients with malignancies of the breast, prostate, lungs, thyroid, or kidneys suffer from severe bone pain due to metastases of the cancer in the skeletal tissue (1, 2). Although several interventions such as analgesics, bisphosphonates, hormone therapy, and systemic radionuclide therapy are available to manage bone pain, these treatments are known to have many undesirable secondary effects on the patient (2). Radiopharmaceuticals containing nuclides such as strontium-89 (as ^89^SrCl_2_) and samarium-153 (administered as ^153^Sm-labeled ethylenediamine tetramethylene phosphonic acid (EDTMP)), which have been approved by the United States Food and Drug Administration (FDA) for the treatment of bone pain due to metastases, are commonly used for the palliative care (http://www.who.int/cancer/palliative/definition/en/) of bone pain in cancer patients (2). However, these are not ideal agents to treat bone pain because the radionuclide either has a long half-life and generates high-energy β^–^ particles (^89^Sr has a half-life of ~50 days; E_β(max)_ = 1.49 MeV) or is short-lived and has to be produced in close vicinity to the treatment center (^153^Sm has a half-life of ~47 h; E_β(max)_ = 0.81 MeV; Eγ = 103 keV (28%)) (1). A major limitation of using these bone pain palliative agents is that they produce myelotoxicity in some patients (3). Between the two labeled compounds, ^89^SrCl_2_ appears to be the agent of choice for clinical applications because its longer half-life allows some flexibility to develop a suitable treatment regimen for the patient. There is great interest in the development of alternative radiolabeled compounds that can be used to treat pain resulting from osseous metastases (2). An important characteristic of a new labeled compound is that it must have the ability to be targeted specifically to the cancerous lesions on the skeleton and should be minimally toxic to the bone marrow as discussed elsewhere (3-5).

In a study with healthy rats, it was reported that EDTMP labeled with lutetium-177 ([^177^Lu]-EDTMP) was cleared rapidly from blood circulation, showed little uptake in the soft tissues, and accumulated primarily in the bones of these animals (6). Chakraborty et al. made similar observations when they investigated the biodistribution of [^177^Lu]-EDTMP in rats (7), and a freeze-dried kit for the preparation of this radiopharmaceutical has also been developed (8). On the basis of these observations, there is a renewed interest to use ^177^Lu (half-life, ~7 days; E_β(max)_ = 497 keV; Eγ = 113 keV (6.4%); 208 keV (11%)) as an alternative nuclide to those currently in use (^89^Sr and ^153^Sm) in the development of a palliative care agent for pain due to the metastases of cancer to the skeletal tissue (4, 5). The main advantages of using ^177^Lu are that it can be easily transported to places where it is not available, and the low-energy gamma photons emitted by the nuclide allow detection of the bone lesions with scintigraphy. The International Atomic Energy Agency has initiated projects to develop ^177^Lu-labeled compounds as palliative care agents for bone pain (5).

Methylene diphosphonate (MDP; also known as methylene diphosphate) labeled with technetium-99m is a commonly used bone-imaging agent approved by the FDA to investigate osteogenesis (http://ghr.nlm.nih.gov/glossary=osteogenesis), and it is commercially available in the form of a kit (9). Because of its easy availability, and on the basis of the information mentioned above, Abbasi developed ^177^Lu-labeled MDP ([^177^Lu]-MDP) as a possible alternate radiopharmaceutical for the palliative care of bone pain (10). The biodistribution of this tracer was studied in Sprague-Dawley rats and confirmed with gamma planar imaging.

### Other Sources of Information

Methylene diphosphonate (MDP)-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=MDP+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=MDP) with MDP and related compounds (with or without radionuclide labeling)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=bone+pain) for bone pain treatment

Rat aminoacyl tRNA synthetase protein (http://www.ncbi.nlm.nih.gov/protein/NP_446209.1) and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/NM_053757.1) sequences

Gene information (http://www.ncbi.nlm.nih.gov/sites/nuccore?Db=gene&DbFrom=nuccore&Cmd=Link&LinkName=nuccore_gene&IdsFromResult=75832034) regarding rat aminoacyl-tRNA synthetase (GeneID: 114632) (Source: Entrez Gene)

Aminoacyl tRNA synthetase in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim?term=aminoacyl%20tRNA%20synthetase)

Structure (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=80673) of human cytosolic phenylalanyl tRNA synthase (Source: NCBI)

Bone palliative agents on the FDA site (http://google2.fda.gov/search?q=bone+palliative+agents&spell=1&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&ie=UTF-8&access=p)

FDA-approved clinical trials with EDTMP (http://clinicaltrials.gov/ct2/results?term=EDTMP), ^89^SrCl_2_ (http://clinicaltrials.gov/ct2/results?term=Strontium+chloride), and ^153^Sm (http://clinicaltrials.gov/ct2/results?term=Sm-153) complexes

Clinical trials with other bone-imaging agents (http://clinicaltrials.gov/ct2/results?term=Bone+imaging)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-MDP%20synthesis&cmd=DetailsSearch)]

A freeze-dried kit of MDP was used to optimize the production of [^177^Lu]-MDP as described by Abbasi (10). The efficiency of the labeling reaction and the radiochemical purity of the final product were both >99% as determined with thin-layer chromatography. The R_f_ values for [^177^Lu]-MDP and ^177^LuCl_3_ were reported to be 0.82 ± 0.04 and zero, respectively, as determined with paper chromatography. Specific activity of the radiolabeled compound was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-MDP%20in%20vitro&cmd=DetailsSearch)]

The in vitro stability of [^177^Lu]-MDP was determined by incubating the tracer at room temperature from 1 min to 92 h as described by Abbasi (10). The labeled compound was reported to have 100% stability for ~22 h, which decreased to ~80% by 92 h. Stability of the probe in rodent or human serum under in vitro conditions was not reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-MDP%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^177^Lu]-MDP was studied in Sprague-Dawley rats (n = 3 animals/time point) as detailed elsewhere (10). The animals were given an intravenous injection of the tracer (~18.5 MBq (~0.5 mCi)) and euthanized at predetermined time points from 2 min to 22 h. Accumulated radioactivity in the major organs, including the femur, was measured as described, and the data were presented as percent uptake of injected dose per gram tissue (% ID/g). The accumulation of radioactivity in the femur increased from 0.56 ± 0.02% ID/g at 1 h postinjection (p.i.) to 1.33 ± 0.04% ID/g at 2 h p.i. and 2.26 ± 0.02% ID/g at 22 h p.i. During this period, the liver showed a nearly constant level of radioactivity (~6.3% ID/g), and the tracer level in the lungs decreased from 31.63 ± 0.97% ID/g at 1 h p.i. to 1.3 ± 1.06% ID/g at 22 h p.i. In the kidneys, accumulation of the probe decreased from 0.51 ± 0.06% ID/g at 1 h p.i. to 0.25 ± 0.05% ID/g at 22 h p.i. The total uptake in the skeleton was calculated to be 8.18 ± 0.05% ID at 1 h p.i. and increased to 31.29 ± 1.27% ID at 22 h p.i. (see calculation details in Abbasi (10)).

Gamma planar imaging of anesthetized rats (n = 2 animals) at 22 h p.i. confirmed that the radioactivity was present primarily in the skeletal tissue of the rodents, followed by the liver as observed during the biodistribution studies (10).

From this study, the investigators concluded that [^177^Lu]-MDP accumulated mainly in the skeletal tissue of the rats, and, except in the liver, little uptake was observed in other soft tissue (10).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-MDP%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-MDP%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=177Lu-MDP%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Das T., et al. (2009). (170)Tm-EDTMP: a potential cost-effective alternative to (89)SrCl(2) for bone pain palliation. Nucl Med Biol.
2 Paes F.M., Serafini A.N. (2010). Systemic metabolic radiopharmaceutical therapy in the treatment of metastatic bone pain. Semin Nucl Med.
3 Jansen D.R., et al. (2010). Targeted radiotherapy of bone malignancies. Curr Drug Discov Technol.
4 Chakraborty S., et al. (2008). 177Lu-EDTMP: a viable bone pain palliative in skeletal metastasis. Cancer Biother Radiopharm.
5 Mathe D., et al. (2010). Multispecies animal investigation on biodistribution, pharmacokinetics and toxicity of 177Lu-EDTMP, a potential bone pain palliation agent. Nucl Med Biol.
6 Ando A., et al. (1998). 177Lu-EDTMP: a potential therapeutic bone agent. Nucl Med Commun.
7 Chakraborty S., et al. (2002). 177Lu labelled polyaminophosphonates as potential agents for bone pain palliation. Nucl Med Commun.
8 Garnuszek P., et al. (2003). Evaluation of a freeze-dried kit for EDTMP-based bone-seeking radiopharmaceuticals. Appl Radiat Isot.
9 . Bracco, Kit for the preparation of technetium Tc 99m Medronate. 2006, Bracco Diagnostics Inc.: Princeton, NJ 08543.
10 Abbasi I.A. (2011). Studies on (177)Lu-labeled methylene diphosphonate as potential bone-seeking radiopharmaceutical for bone pain palliation. Nucl Med Biol.